# Anti-malondialdehyde-modified low-density lipoprotein MDA2 monoclonal antibody–labeled lipid-coated ultra-small superparamagnetic iron oxide nanoparticles

Chemical name: | Anti-malondialdehyde-modified low-density lipoprotein MDA2 monoclonal antibody–labeled lipid-coated ultra-small superparamagnetic iron oxide nanoparticles
Abbreviated name: | MDA2 LUSPIOs
Synonym:
Agent category: | Antibody
Target: | Malondialdehyde-modified low-density lipoprotein (MDA-LDL)
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=44888831), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=217035086) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=338) for more information about apolipoprotein B.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Apolipoprotein E (apoE) is essential for the normal catabolism of triglyceride-rich lipoprotein chylomicrons (lipoprotein particles) (2). Oxidation of low-density lipoprotein (LDL) generates a number of highly reactive short chain-length aldehydic fragments of oxidized fatty acids capable of conjugating with lysine residues of apoliprotein B and other proteins. Oxidized LDL is present in atherosclerotic lesions and is essential for formation of foam cells in atherosclerotic plaques. During atherogenic conditions, depositions of lipids and extracellular matrix proteins on the endothelial cell surfaces of the aorta and cells lead to the development of atherosclerotic plaques (3), which may erode and rupture. MDA2 is a murine monoclonal antibody to malondialdehyde-lysine epitopes of MDA-LDL and other oxidatively modified proteins but not to normal LDL (4). Briley-Saebo et al. (5) showed accumulation of MDA2 micelles containing Gd (MDA2-Gd micelles) in macrophages of atherosclerotic lesions in apoE-deficient (apoE^–/–^) mice using MRI. However, Gd may lead to renal toxicity in patients. In another study, Briley-Saebo et al. (6) conjugated MDA2 antibody to lipid-coated ultra-small superparamagnetic iron oxide nanoparticles (LUSPIOs) for in vivo detection of atherosclerotic lesions in apoE^–/–^ mice using MRI.

### Related Resource Links:

- Chapters in MICAD (MDA (http://www.ncbi.nlm.nih.gov/books?term=malondialdehyde%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (apolipoprotein E (http://www.ncbi.nlm.nih.gov/gene/348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (apolipoprotein E (http://omim.org/entry/107741))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+synthesis)]

USPIOs coated with polyethylene glycol (PEG) were commercially available (Clariscan, Amersham/GE Health Care). 1,2-Distearoyl-sn-glycer-3-phosphoethanolamine-n-methoxy(polyethylene glycol-2000 (PEG-DSPE) and PEG-malamide-DSPE were added to USPIOs at a ratio of 17.3 mg:1.3 mg per mg Fe in a chloroform solution, with rhodamine added as a fluorescent label (6). The solution was added stepwise to boiling HEPES buffer (pH 7) under vigorous stirring until a clear brown solution was formed. LUSPIOs were isolated with ultracentrifugation. MDA2 (2.3 nmol/mg Fe) was modified with S-acetylthioglycolic acid N-hydroxysuccinimide ester and then covalently linked to the surface of LUSPIOs. MDA2 LUSPIOs have a hydrated diameter (HD) of 14 ± 3 nm with an r1 value of 13 nM^–1^s^–1^ and an r2 value of 37 nM^–1^s^–1^ at 60 MHz and 40ºC. Untargeted LUSPIOs have a HD of 10 ± 3 nm with an r1 value of 14 nM^–1^s^–1^ and an r2 value of 35 nM^–1^s^–1^ at 60 MHz and 40ºC. Only one in every sixteen LUSPIOs contained an MDA2 antibody. MDA2 LUSPIOs exhibited <5% variation in size and/or r2/r1 values at 4°C for 30 d.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+in+vitro)]

Confocal microscopy analysis showed accumulation of MDA2 LUSPIOs (1 mM Fe) in MDA-LDL–pretreated J7774A.1 macrophages, whereas no accumulation (non-detectable) was observed with untargeted LUSPIOs (1 mM Fe concentration in the solution added to the cells) (6). The Fe content was 0.31 pg/cell for MDA2 LUSPIOs and non-detectable for untargeted LUSPIOs. The accumulation of dextran-coated Feridex (positive untargeted control, HD = 40 nm) by the macrophages was 1.9 Fe pg/cell; thus, the PEG-coating of LUSPIOs limited their accumulation by the macrophages. If every MDA2-LUSPIO contained MDA2 antibody, a theoretical accumulation of 5–6 pg Fe/cell was expected.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+rodentia)]

Briley-Saebo et al. (6) performed in vivo T2* MRI (9.4 T) studies of MDA2 LUSPIOs in 10-month-old apoE^–/–^ knockout mice that were fed a high-fat, high-cholesterol diet at 6 weeks of age and 10-month-old wild-type normal mice on normal diet at 0 h and 24 h after injection. Animals were injected with either 3.9 mg Fe/kg MDA2 LUSPIOs (n = 9 apoE^–/–^ mice or 5 wild-type mice) or LUSPIOs (n = 5 apoE^–/–^ mice or 5 wild-type mice). There was a significant loss (60%) of R2* value in the atherosclerotic lesions of the apoE^–/–^ aorta with MDA2 LUSPIOs (P < 0.003) but not with untargeted LUSPIOs. Co-injection of 20 nmol MDA2 antibody inhibited the loss of R2* value by 75% (P < 0.0002). The loss of R2* value for MDA2 LUSPIOs was not observed in the aorta of the wild-type mice. The liver accumulation was 25% and 31% injected dose for MDA2 LUSPIOs and LUSPIOs, respectively. The blood half-lives were 9.01 h and 1.52 h for MDA2 LUSPIOs and LUSPIOs in apoE^–/–^ mice, respectively. On the other hand, the blood half-lives (1.55 h versus 1.41 h) were similar in the wild-type mice. Confocal microscopy revealed that MDA2 LUSPIOs colocalized primarily with CD68 staining (macrophages) in atherosclerotic lesions in the arterial wall. Immunochemistry showed a strong co-localization of Fe content and MDA-lysine epitopes in the atherosclerotic plaques. A similar loss of R2* signal was also observed with a human single-chain Fv antibody fragment IK17 targeted to MDA-like epitopes (IK17-LUSPIOs) and a natural IgM autoantibody (E06) cloned from apoE^–/–^ mice that binds to the phosphocholine head group of oxidized phospholipids (E06 LUSPIOs).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+human)]

No publication is currently available.

## NIH Support

R01 EB009638, R01 EB009638-07, R01 HL071021-07, R01 HL078667-04S1, R01 HL71021, R01 HL78667, R21 HL091399-01A2, R21 HL091399-02

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Eichner J.E., Dunn S.T., Perveen G., Thompson D.M., Stewart K.E., Stroehla B.C. (2002). Apolipoprotein E polymorphism and cardiovascular disease: a HuGE review. Am J Epidemiol.
3 Libby P. (2002). Inflammation in atherosclerosis. Nature.
4 Palinski W., Yla-Herttuala S., Rosenfeld M.E., Butler S.W., Socher S.A., Parthasarathy S., Curtiss L.K., Witztum J.L. (1990). Antisera and monoclonal antibodies specific for epitopes generated during oxidative modification of low density lipoprotein. Arteriosclerosis.
5 Briley-Saebo K.C., Shaw P.X., Mulder W.J., Choi S.H., Vucic E., Aguinaldo J.G., Witztum J.L., Fuster V., Tsimikas S., Fayad Z.A. (2008). Targeted molecular probes for imaging atherosclerotic lesions with magnetic resonance using antibodies that recognize oxidation-specific epitopes. Circulation.
6 Briley-Saebo K.C., Cho Y.S., Shaw P.X., Ryu S.K., Mani V., Dickson S., Izadmehr E., Green S., Fayad Z.A., Tsimikas S. (2011). Targeted iron oxide particles for in vivo magnetic resonance detection of atherosclerotic lesions with antibodies directed to oxidation-specific epitopes. J Am Coll Cardiol.